# ^89^Zr-Labeled p-isothiocyanatobenzyl-desferrioxamine B (Df-Bz-NCS)–conjugated panitumumab, a fully human monoclonal antibody directed against the extracellular domain III of the epidermal growth factor receptor

Chemical name: | ^89^Zr-Labeled p-isothiocyanatobenzyl-desferrioxamine B (Df-Bz-NCS)–conjugated panitumumab, a fully human monoclonal antibody directed against the extracellular domain III of the epidermal growth factor receptor
Abbreviated name: | [^89^Zr]-Panitumumab
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor (EGFR) extracellular domain III
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=panitumumab&cmd=DetailsSearch)]

Panitumumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=e0fa4bca-f245-4d92-ae29-b0c630a315c2) is a fully human anti-epidermal factor receptor 1 (HER1) monoclonal antibody (mAb) that has been approved by the United States Food and Drug Administration (FDA) for the treatment of metastatic colorectal cancers (http://cancer.gov/cancertopics/wyntk/colon-and-rectal) that express the EGFR and are unresponsive to chemotherapy (1). This mAb has a very high affinity for the extracellular domain III of the HER1. The mode of action of panitumumab has been illustrated by Dubois and Cohen (1), and the general characteristics of this mAb have been described by Argiles et al. (2). The fully human mAb is well tolerated by individuals, slows disease progression, and improves the progression-free survival of patients (3). Therefore, ^111^In-labeled panitumumab was evaluated for the noninvasive detection of HER1-positive tumors in an effort to screen for patients who would benefit most from radioimmunotherapy with this mAb after labeling it with a suitable high-energy radionuclide (3). ^64^Cu-Labeled panitumumab has been used with positron emission tomography (PET) for the detection of head and neck squamous cell carcinoma xenograft tumors (these tumors express high levels of HER1) in mice, and it has been shown that only low levels of the labeled mAb accumulated in the lesions (4). The low uptake of the radiolabeled mAb by the tumors is attributed to poor vascular permeability of the lesions. Immunohistochemistry is the method of choice to quantify expression of the HER family of receptors in cancerous lesions, but results obtained with this technique do not establish a clear correlation between the response to anti-HER1 immunotherapy and the level of HER1 in the cancerous lesions (5). In other studies, ^86^Y-labeled panitumumab ([^86^Y]-panitumumab) was used with PET to detect HER1-positive tumors in mice (6). It has also been shown that [^86^Y]-panitumumab is superior to [^86^Y]-cetuximab for determination of the HER1 status of malignant mesothelioma in mice (7). However, ^64^Cu and ^86^Y have half-lives of 12.7 h and 14.7 h, respectively, which may limit the imaging and quantification of tumors that express the HER1 beyond 3 days postinjection (p.i.) (8). Nayak et al. proposed that ^89^Zr would be a more suitable radionuclide than either ^64^Cu or ^86^Y to detect or quantify HER1 in tumors with PET because ^89^Zr has a half-life of 78.4 h and can be followed in the clinic for more than one week (8). Moreover, ^89^Zr-labeled trastuzumab was used successfully with PET to visualize and quantify HER2-positive metastatic breast cancer lesions and has been shown to produce better quality high spatial resolution images compared with ^111^In-labeled trastuzumab (9).

Nayak et al. studied the biodistribution of ^89^Zr-labeled panitumumab ([^89^Zr]-panitumumab) in mice bearing xenograft LS-174T (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CL-188&Template=cellBiology) cell tumors (human colorectal adenocarcinoma cells that express the HER1) and evaluated its utility to visualize HER1-positive tumors with PET in different animal models of metastatic cancer (8).

### Related Resource Links

Panitumumab-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Panitumumab%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

EGFR-related chapters (http://www.ncbi.nlm.nih.gov/books/?term=EGFR+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

EGFR (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=EGFR&Submit=Go) (in Pathways Interaction Database)

EGFR in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/131550))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Panitumumab) with panitumumab

Other anti-EGFR antibodies approved for clinical use by the FDA (cetuximab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=8bc6397e-4bd8-4d37-a007-a327e4da34d9), trastuzumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=492dbdb2-077e-4064-bff3-372d6af0a7a2))

EGFR tyrosine kinase inhibitors [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EGFR%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-panitumumab%20synthesis&cmd=DetailsSearch)]

Panitumumab (obtained from a source) was conjugated with p-isothiocyanatobenzyl-desferrioxamine B, a bifunctional chelate, for labeling with ^89^Zr as described by Nayak et al. (8). The chelate/protein ratio was reported to be 1.7 ± 0.3 as determined with the isotope dilution method (8). The mAb was labeled with ^89^Zr-oxalate, and the labeled product was purified with a PD-10 desalting column. The radiochemical yield of the labeling reaction ranged from 80% to 95%, and the highest specific activity of [^89^Zr]-panitumumab was 2.0–2.5 GBq/66.66 nmol (54.05–67.56 mCi/66.66 nmol). The radiochemical purity and stability of the final product were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-panitumumab%20in%20vitro&cmd=DetailsSearch)]

A fixed cell binding assay (the type of cells used for the assay was not mentioned) demonstrated that [^89^Zr]-panitumumab had a binding specificity of 72.39 ± 5.23% and showed a nonspecific binding of 5.03 ± 2.33% (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-panitumumab%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^89^Zr]-panitumumab was studied in groups of mice bearing subcutaneous LS-174T cell or A375 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1619&Template=cellBiology) cell (human melanoma cells that do not express the HER1; negative controls) xenograft tumors as described by Nayak et al. (8). The animals (n = 5 mice/time point per group) were injected intravenously with 0.4–0.6 MBq (10.8–16.2 μCi; <33.33 pmol) [^89^Zr]-panitumumab, and the rodents were euthanized at various time points ranging from 1 d to 9 d to recover the major organs and to determine the amount of radioactivity accumulated in the different tissues. Results obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). Among all the tissues, maximum accumulation of radioactivity was observed in the tumors during the entire course of the study (27.92 ± 3.47% ID/g, 42.89 ± 4.49% ID/g, and 25.65 ± 1.73% ID/g at 1, 3, and 9 d p.i., respectively). The amount of tracer in the blood decreased from 11.47 ± 1.37% ID/g at 1 d p.i. to 3.25 ± 0.34% ID/g at 9 d p.i. (a 3.5-fold decrease). A similar trend was noticed in the liver (9.02 ± 0.29% ID/g at 1 d p.i. and decreased to 2.18 ± 0.20% ID/g by 9 d p.i.; a 4.2-fold decrease). The tumor/blood (T/B) ratio increased from 2.4 at 1 d p.i. to 7.9 at 9 d p.i. (a 3.3-fold increase). An increase in uptake of the label was observed in the bone (femur) from 1 d p.i. (1.58 ± 0.17% ID/g) to 9 d p.i. (6.94 ± 0.17% ID/g), indicating that ^89^Zr had a tendency to accumulate in this tissue. To establish receptor binding specificity of the radioimmunoconjugate, another group of mice (n = 5 animals/cell type) bearing the two different cell type tumors were injected with a mixture of [^89^Zr]-panitumumab and 66.66 nmol nonradioactive panitumumab (8). The animals were subsequently euthanized at 6 d p.i. to determine the uptake of radioactivity in the various tissues. The amount of label in the tumors of these rodents decreased significantly (P ≤ 0.001) from 32.14 ± 1.41% ID/g at 1 d p.i. to 6.98 ± 0.52% ID/g at 6 d p.i., indicating that the labeled mAb had a high binding specificity for the receptor. During the study, no change in uptake of radioactivity was observed in the cancerous lesions or in any normal tissues of animals bearing the A375 cell tumors.

In another study, the biodistribution of [^89^Zr]-panitumumab was studied in groups of mice with disseminated intraperitoneal metastatic LS-174T cell carcinomas (8). The animals were given an intraperitoneal injection of the labeled mAb as detailed above, and the mice were euthanized at different time points ranging from 1 d p.i. to 7 d p.i. to determine the amount of radioactivity present in the major organs. The uptake of tracer in the tumor decreased from 96.58 ± 8.97% ID/g at 1 d p.i. to 17.17 ± 3.09% ID/g at 7 d p.i. The amount of radioactivity in blood circulation decreased from 12.85 ± 1.22% ID/g at 1 d p.i. to 0.42 ± 0.06% ID/g at 7 d p.i During the same period, the T/B ratio increased from 7.5 at 1 d p.i. to 41.6 at 7 d p.i. (>5-fold increase). The uptake of label in the bone increased from 3.00 ± 0.37% ID/g at 1 d p.i. to 7.00 ± 1.32% ID/g at 7 d p.i., once again indicating that ^89^Zr had a tendency to accumulate in this tissue. No blocking studies were reported.

Mice with metastatic pulmonary colorectal carcinoma tumors derived from LS-174T cells were also used to study the biodistribution of [^89^Zr]-panitumumab (8). The animals (n = 5 mice/time point) were injected with the radioimmunoconjugate as before and euthanized at predetermined time points ranging from 1 d p.i. to 5 d p.i. to retrieve the organs of interest and the tumors as described above. The peak uptake of radioactivity in the tumor was 78.05 ± 7.15% ID/g at 2 d p.i. and decreased to 61.97 ± 6.02% ID/g by 5 d p.i. During the same period, the amount of label in the blood decreased from 11.11 ± 0.73 at 2 d p.i. to 3.70 ± 0.42% ID/g at 5 d p.i., and the T/B ratio increased from 7.09 ± 0.64 at 2 d p.i. to 17.26 ± 2.05 at 5 d p.i. Mice coinjected with [^89^Zr]-panitumumab and 66.66 nmol nonradioactive panitumumab showed an uptake of only 11.61 ± 1.26% ID/g at 5 d p.i. (compared with 61.97 ± 6.02% ID/g at the same time point in mice without the blocking dose), which indicated that the labeled mAb bound specifically to the target receptor.

For PET imaging, mice bearing subcutaneous LS-174T cell tumors (the number of animals used in the study was not reported) were injected with 1.7–1.9 MBq (45.9–51.3 μCi; <33.33 pmol) [^89^Zr]-panitumumab through the tail vein (8). Another group of mice bearing subcutaneous tumors were coinjected with the radiolabeled mAb and a blocking dose (66.66 nmol) of the nonradioactive mAb. PET images of both groups of animals were acquired at 1 d p.i., 3 d p.i., and 6 d p.i. The tumors were clearly visible at all time points only in the PET images of rodents injected with the labeled mAb alone, whereas the lesions were barely visible in animals that received the blocking dose of the mAb. This study once again established that [^89^Zr]-panitumumab had a binding specificity for HER1. From time-activity curves it was calculated that the average amount of radioactivity in the HER1-positive tumors over the 6-d period was 204.13 ± 9.67% ID/d per gram tissue (% ID/d per g), which was significantly higher (P < 0.001) than the accumulation in the LS-174T tumors obtained from mice coinjected with a blocking dose of nonradioactive panitumumab (36.45 ± 1.39% ID/d per g). In addition, the uptake values for the tumors and the liver that were observed during the biodistribution study correlated well with values calculated from the PET images (r^2^ = 0.95; P = 0.97).

Whole-body PET imaging of mice bearing intraperitoneal LS-174T tumors given an intraperitoneal injection of [^89^Zr]-panitumumab as before revealed that at 1 d p.i. the radioactivity accumulated primarily along the peritoneal walls and the liver lobes of the animals (8). At this time point, the label was also visible in the blood pool (heart and lungs) of the animals. By 5 d p.i., the tracer had cleared from the blood pool and was present mainly around the peritoneal wall and the liver lobes. The presence of tumor nodules along the peritoneal walls and the liver lobes of the animals where the radioactivity was observed to have accumulated in the PET images was confirmed with T_2_-weighted MRI and postmortem dissection of the animals.

Mice bearing metastatic pulmonary LS-174T cell tumors were also subjected to PET imaging and T_2_-weighted MRI as described above (8). From the PET images it was evident that the radioactivity was present mainly in the blood pool and the left thoracic area of the animals at 1 d p.i. The label cleared from the blood pool by 5 d p.i., and the tracer was present primarily in the left thoracic cavity area at this time point. MRI of the animals at 5 d p.i. showed that the tumors were present in the left corner of the thoracic region where the radioactivity was seen to have accumulated in the PET images.

From these studies, the investigators concluded that [^89^Zr]-panitumumab was suitable for the determination of the HER1 status of metastatic tumors in rodents (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-panitumumab%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-panitumumab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-panitumumab%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Work presented in this chapter was supported by the Intramural Research Program of the National Institutes of Health, National Cancer Institute, and the Center for Cancer Research.

## References

1 Dubois E.A., Cohen A.F. (2009). Panitumumab. Br J Clin Pharmacol.
2 Argiles G., Dienstmann R., Elez E., Tabernero J. (2012). Panitumumab: a summary of clinical development in colorectal cancer and future directions. Future Oncol.
3 Ray G.L., Baidoo K.E., Wong K.J., Williams M., Garmestani K., Brechbiel M.W., Milenic D.E. (2009). Preclinical evaluation of a monoclonal antibody targeting the epidermal growth factor receptor as a radioimmunodiagnostic and radioimmunotherapeutic agent. Br J Pharmacol.
4 Niu G., Li Z., Xie J., Le Q.T., Chen X. (2009). PET of EGFR antibody distribution in head and neck squamous cell carcinoma models. J Nucl Med.
5 Yonemori K., Tsuta K., Shimizu C., Hatanaka Y., Hirakawa A., Ono M., Kouno T., Katsumata N., Ando M., Tamura K., Hasegawa T., Kinoshita T., Fujiwara Y. (2010). Immunohistochemical expression of HER1, HER3, and HER4 in HER2-positive breast cancer patients treated with trastuzumab-containing neoadjuvant chemotherapy. J Surg Oncol.
6 Nayak T.K., Garmestani K., Baidoo K.E., Milenic D.E., Brechbiel M.W. (2010). Preparation, biological evaluation, and pharmacokinetics of the human anti-HER1 monoclonal antibody panitumumab labeled with 86Y for quantitative PET of carcinoma. J Nucl Med.
7 Nayak T.K., Garmestani K., Milenic D.E., Baidoo K.E., Brechbiel M.W. (2011). HER1-targeted 86Y-panitumumab possesses superior targeting characteristics than 86Y-cetuximab for PET imaging of human malignant mesothelioma tumors xenografts. PLoS One.
8 Nayak T.K., Garmestani K., Milenic D.E., Brechbiel M.W. (2012). PET and MRI of metastatic peritoneal and pulmonary colorectal cancer in mice with human epidermal growth factor receptor 1-targeted 89Zr-labeled panitumumab. J Nucl Med.
9 Dijkers E.C., Oude Munnink T.H., Kosterink J.G., Brouwers A.H., Jager P.L., de Jong J.R., van Dongen G.A., Schroder C.P., Lub-de Hooge M.N., de Vries E.G. (2010). Biodistribution of 89Zr-trastuzumab and PET imaging of HER2-positive lesions in patients with metastatic breast cancer. Clin Pharmacol Ther.